# Ultrasmall superparamagnetic iron oxide-Leu-Ile-Lys-Lys-Pro-Phe

Chemical name: | Ultrasmall superparamagnetic iron oxide-Leu-Ile-Lys-Lys-Pro-Phe
Abbreviated name: | USPIO-R826
Synonym:
Agent category: | Peptide
Target: | Phosphatidylserine (PS)
Target category: | Acceptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-R826)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, the paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells like epithelial cells and immune cells (2). During apoptosis, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. PS is also accessible for annexin V binding in apoptosis and necrosis because of disruption of the plasma membrane. Annexin V binds to PS with high affinity (dissociation constant = 7 nM). Annexin V has been radiolabeled with ^123^I, ^124^I, and ^99m^Tc for use with single-photon emission computed tomography and positron emission tomography imaging (PET) (3-5). Recently, annexin V was successfully labeled with ^18^F (6, 7), and ^18^F-labeled annexin V is being developed as a PET agent for imaging apoptosis as well as necrosis. Cy5.5-annexin V and quantum dot (QD)-annexin V (8) have been evaluated as optical probes for near-infrared (NIR) imaging. Various bimodal annexin V–conjugated nanoparticles have been developed for imaging apoptosis, such as annexin V-CLIO-Cy5.5 and annexin V-QD-gadolinium for use with NIR and MRI imaging (9, 10).

A cyclic peptide, Cys-Leu-Ile-Lys-Lys-Pro-Phe-Cys, was identified with phage screening against PS (11). A linear peptide, Leu-Ile-Lys-Lys-Pro-Phe (P826), was synthesized and conjugated to the 8-amino-3,6-dioxaoctanoyl linker to form g-R826, which was conjugated with 2-(4-isothiocyanatobenzyl)-diethylenetriamine pentaacetic acid (p-SCN-Bn-DTPA) to form DTPA-g-R826 for labeling with Gd (Gd-DTPA-g-R826) for MRI of PS in apoptosis. Gd-DTPA-g-R826 was validated on apolipoprotein E–deficient (apoE−^/^−) mice with in vivo MRI for characterization of atherosclerotic plaque. However, Gd-DTPA-g-R826 exhibited low MRI efficacy (low r_1_ and r_2_ relaxivity values). Burtea et al. (12) prepared ultrasmall superparamagnetic iron oxide-R826 (USPIO-R826) for use with MRI of PS in apoptosis for characterization of atherosclerotic plaques.

### Related Resource Links:

- Chapters in MICAD (Annexin V (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Annexin%20V+AND+micad%5Bbook%5D))
- Gene information in NCBI (Annexin V (http://www.ncbi.nlm.nih.gov/gene/308))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Annexin V (http://www.ncbi.nlm.nih.gov/omim/131230))
- Clinical trials (Annexin V (http://www.clinicaltrials.gov/ct2/results?term=Annexin+V+))
- Drug information in FDA (Annexin V (http://google2.fda.gov/search?q=annexin+V&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-R826%20and%20synthesis)]

R826 peptide (with two Lys, protected by reaction with trifluoroacetic acid to form amides, and attached to 8-amino-3,6-dioxaoctanoyl at the N-terminus) and N-(3-dimethylaminopropyl)-N'-ethylcarbodiimide hydrochloride (EDCI) were added to USPIO nanoparticles and incubated for 20 h (12). The nanoparticles were isolated with ultrafiltration. A solution of the nanoparticles, EDCI, and aminoPEG750 was incubated for 17 h. The peptide was deprotected by hydrolysis (pH 10) for 6 h at room temperature. The product, USPIO-R826, was isolated with ultrafiltration. A nonspecific peptide (NSP) was also similarly conjugated to USPIO for use as control. The hydrodynamic diameters of USPIO-R826, USPIO-NSP, and USPIO-PEG were 26–27 nm. USPIO-R826, USPIO-NSP, and USPIO-PEG exhibited longitudinal (r_1_) relaxivity values of 1.9–2.4 mM−^1^s−^1^ at 7 T, and transverse (r_2_) relaxivity values of 88.8, 75.6, and 74.6 mM−^1^s−^1^ at 7 T, respectively. The number of peptides per USPIO-R826 nanoparticle was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-R826%20and%20in%20vitro)]

Burtea et al. (12) performed in vitro saturation binding assays with various concentrations of USPIO-R826, which exhibited a K_d_ value of 774 nM, to determine the agent's binding affinity to immobilized PS. In vitro cellular accumulation assays of USPIO-R826 (774 nM, 4 mM Fe) and USPIO-PEG (4 mM Fe) were performed in human Jurkat T cells before and after treatment with camptothecin to induce apoptosis_._ The cellular Fe level of USPIO-R826 was 426% higher in the treated cells than that in the nontreated cells and seven- to eight-fold higher than that of USPIO-PEG.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-R826%20and%20rodentia)]

Burtea et al. (12) performed in vivo 4.7-T MRI in apoE−^/^− mice (n = 6) before and after injection with 0.1 mmol Fe/kg USPIO-R826, USPIO-NSP, or USPIO-PEG. There was −50% contrast in MRI signal intensity (ΔSNR) in the aortic wall at 52 min after injection of USPIO-R826. The aortic ΔSNR remained constant for up to 92 min of imaging and decreased to −39% at 24 h. The liver signals were −47% and −31% at 32 min and 24 h, respectively. UPSIO-NSP exhibited aortic ΔSNR of −20% during the 92-min scans and decreased to −16% at 24 h. The liver signals were −11%, −20%, and −33% at 33 min, 92 min, and 24 h, respectively. USPIO-PEG produced aortic ΔSNR of −37% and −6% at 221 min and 24 h, respectively. The liver signals were 4%, 12%, and −30% at 33 min, 92 min, and 24 h, respectively. USPIO-R826 provided higher loss of contrast than the two controls (USPIO-NSP and USPIO-PEG). Immunohistological staining of the aorta sections of apoE−^/^− mice confirmed the presence of atherosclerotic lesions with extensive expression of VCAM-1. R826 colocalized with caspase-3 (an apoptotic enzyme) and expression (r^2^ = 0.714). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-R826%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-R826%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO-R826%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
3 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
4 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
5 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
6 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
7 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
8 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
9 Prinzen L., Miserus R.J., Dirksen A., Hackeng T.M., Deckers N., Bitsch N.J., Megens R.T., Douma K., Heemskerk J.W., Kooi M.E., Frederik P.M., Slaaf D.W., van Zandvoort M.A., Reutelingsperger C.P. (2007). Optical and magnetic resonance imaging of cell death and platelet activation using annexin a5-functionalized quantum dots. Nano Lett.
10 van Tilborg G.A., Mulder W.J., Chin P.T., Storm G., Reutelingsperger C.P., Nicolay K., Strijkers G.J. (2006). Annexin A5-conjugated quantum dots with a paramagnetic lipidic coating for the multimodal detection of apoptotic cells. Bioconjug Chem.
11 Burtea C., Laurent S., Lancelot E., Ballet S., Murariu O., Rousseaux O., Port M., Vander Elst L., Corot C., Muller R.N. (2009). Peptidic targeting of phosphatidylserine for the MRI detection of apoptosis in atherosclerotic plaques. Mol Pharm.
12 Burtea C., Ballet S., Laurent S., Rousseaux O., Dencausse A., Gonzalez W., Port M., Corot C., Vander Elst L., Muller R.N. (2012). Development of a magnetic resonance imaging protocol for the characterization of atherosclerotic plaque by using vascular cell adhesion molecule-1 and apoptosis-targeted ultrasmall superparamagnetic iron oxide derivatives. Arterioscler Thromb Vasc Biol.